# GKVLAK–(Gadolinium-(1,4,7,10-tetraazacyclododecane-1,4,7-tris(acetic acid t-butyl ester)-10-acetic acid monoamide))–GGGGTVQQEL

Chemical name: | GKVLAK–(Gadolinium-(1,4,7,10-tetraazacyclododecane-1,4,7-tris(acetic acid t-butyl ester)-10-acetic acid monoamide))–GGGGTVQQEL | [image]
Abbreviated name: | Gd-DCCP16 | [image]
Synonym: | | [image]
Agent Category: | Peptides | [image]
Target: | Transglutaminases | [image]
Target Category: | Enzymes | [image]
Method of detection: | Magnetic resonance imaging (MRI) | [image]
Source of signal / contrast: | Gadolinium (Gd) | [image]
Activation: | Yes | [image]
Studies: | - In vitro; - Rodents | Structure of Gd-DCCP16 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Transglutaminases%20and%20imaging)]

The gadolinium (Gd)-labeled 16-peptide agent GKVLAK-(Gd-(1,4,7,10-tetraazacyclododecane-1,4,7-tris(acetic acid t-butyl ester)-10-acetic acid monoamide (DOTAMA)))-GGGGTVQQEL, abbreviated as Gd-DCCP16, was developed by Tei et al. for magnetic resonance imaging (MRI) of the pathological processes associated with high transglutaminase activity (1).

Transglutaminases are a family of Ca^2+^-dependent enzymes that catalyze extracellular covalent cross-linking of proteins (2, 3). These enzymes participate in many important biological processes, such as blood coagulation, skin-barrier formation, hardening of the fertilization envelope, and extracellular matrix assembly (2, 4). They are also involved in multiple pathological processes, including wound healing, cancer, myocardial infarctions, and atherothrombosis (5-7). The fibrin-stabilizing factor XIII (FXIII, also known as plasma transglutaminase) and the tissue transglutaminase (TG2) are the two enzymes that have attracted the greatest interest in transglutaminase-targeted imaging and therapy (1, 8, 9). FXIII cross-links fibrin during blood clotting and subsequently produces a mechanically stronger clot with high fibrinolytic resistance, whereas TG2 catalyzes covalent cross-linking of the extracellular matrix. The enzyme-mediated cross-linking is achieved by forming an isopeptide bond between the γ-carbonyl group of a glutamine (Gln) in one protein and the ε-amino group of a lysine (Lys) residue in a nearby protein (3, 9). This cross-link can be blocked by covalent incorporation of an acyl-acceptor amine substrate into the fibrin units or an acyl-donor Gln-containing peptide complementary to the FXIII-reactive Lys donor cross-linking sites of the protein (1). FXIII and TG2 are much more sensitive toward the Gln-bearing substrates than to amine donor Lys residues. These transglutaminase features form the fundamental basis for the development of imaging agents for detection of transglutaminase activity. In recent years, peptides based either on β-casein and α2-antiplasmin for the Gln-donor substrate requirements or on the bovine αA-crystallin for the amine donor substrate requirements have been synthesized for in vitro transglutaminase assays, and imaging probes consisting of peptides from α2-antiplasmin have been investigated for mapping the activity of endogenous FXIII and TG2 (10-12).

Tei et al. designed a new model peptide, DCCP16, which was labeled with Gd for MRI and the fluorescent dye IRIS Blue for optical imaging (1). The DCCP16 peptide consists of two moieties. The first moiety is the hexapeptide TVQQEL, which bears two Gln residues and one valine residue. The second moiety is the pentapeptide GKVLA, which is known to be a good substrate for transglutaminases. A four-glycine spacer and a Lys residue were inserted between the Lys and the Gln moieties for conjugation of the Gd-DOTAMA or the IRIS Blue-DOTAMA. This spacer-DOTAMA was chosen to keep the Gd- or IRIS Blue-complex far enough from interfering with the active site. The MRI and optical probes were therefore set as GKVLAK-(Gd-DOTAMA)-GGGGTVQQEL (Gd-DCCP16) and GKVLAK-(IRIS Blue-DOTAMA)-GGGGTVQQEL (DCCP16-IRIS Blue), respectively. In vivo effectiveness of the two agents was validated with MRI and optical mapping of transglutaminase-induced agent retention in mouse models of tumor xenografts and blood clotting (1). Noninvasive imaging of transglutaminase activity with Gd-DCCP16 or DCCP16-IRIS Blue provides an important tool for detecting and monitoring transglutaminase-targeted therapy in diverse pathologies including cancer, wound healing, myocardial infarction, and pregnancy failure associated with congenital FXIII deficiency (1). This chapter describes the results generated with Gd-DCCP16. The results obtained with DCCP16-IRIS Blue were described in the chapter on DCCP16-IRIS Blue in MICAD.

### Related Resource Links:

- Chapters of FXIII in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Factor%20XIII%20AND%20micad%5bbook%5d)
- Articles of transglutaminases in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/?term=Transglutaminases)
- Nucleotides (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Transglutaminases) and proteins (http://www.ncbi.nlm.nih.gov/protein/?term=Transglutaminases) of transglutaminases
- Bioassays of transglutaminase activity (http://www.ncbi.nlm.nih.gov/pcassay) in PubChem BioAssay

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20812289)]

The DCCP16 peptide GKVLAKGGGGTVQQEL and the DCCP16 control GAVLAKGGGGTVAAEL were synthesized with solid-phase peptide synthesis with a rink amide resin as solid support and the standard Fmoc strategy (1). As the negative control peptide, the amino acids responsible for the transglutaminase activity of DCCP16 (Gln and Lys) were replaced with alanine. DOTAMA was coupled to the ε-NH_2_ group of the Lys residue. The purity values of both GKVLAK-(DOTAMA)-GGGGTVQQEL (DCCP16) and GAVLAK-(DOTAMA)-GGGGTVAAEL (DCCP16 control) were >95%. The yields of DCCP16 and DCCP16 control were 25% (48 mg) and 20% (35 mg), respectively. Chelation with Gd was completed with reactions of GdCl_3_ and DCCP16 or DCCP16 control. Centrifugation was used to remove Gd(OH)_3_ from the reaction solution. Orange Xylenol ultraviolet analysis showed that the residual free Gd^3+^ ion was <0.3% (mol/mol) in both Gd-DCCP16 and Gd-DCCP16 control. The relaxivity of Gd-DCCP16 in water was 8.1 mM^-1^s^-1^ at 0.5 T and 298 K. The relaxivity of Gd-DCCP16 control was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20812289)]

Two in vitro MRI experiments were performed to determine whether Gd-DCCP16 enters into the clot fibrin network (1). ProHance, a commercially available, nonspecific MRI contrast agent, was selected as the control. Different concentrations of Gd (100–400 M) were tested for both Gd-DCCP16 and ProHance. The first experiment was designed to allow the Gd-DCCP16 to enter the clot formation. Clots were formed in a 2-ml vial with reconstituted human plasma and pathromtin SL. After incubation for two min at 37ºC with or without Gd-DCCP16 or ProHance, CaCl_2_ solution was then added to form the clot. The formed clots were washed to remove the unbound agent and then placed in a 1.5-ml vial for MRI measurements. Notable signal enhancement was observed on clot preparation in which Gd-DCCP16 was part of the clot structure, whereas only a small enhancement was detectable on clots prepared in the presence of ProHance. The second experiment was designed to evaluate the noncovalent interaction between the Gd-DCCP16 and the preformed clot. No evident enhancement was observed when either Gd-DCCP16 or ProHance was incubated with preformed clots. The signal enhancement in MRI images from the first experiment reflected the formation of covalent bonds between the peptide and fibrin, in which Gd-DCCP16 entered into the clot fibrin network as a fibrinogen mimetic. The data in the second experiment suggested the absence of noncovalent interaction between DCCP16 and the preformed clot.

To further verify whether Gd-DCCP16 is covalently linked by transglutaminase activity, large MCF7 (human breast cancer cell line) spheroids (1 mm in diameter) were generated and incubated for 48 h with Gd-DCCP16 (1). Contrast enhancement was observed in T1-weighted images of spheroids incubated with Gd-DCCP16 in comparison to control spheroids.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20812289)]

In vivo contrast enhancement with Gd-DCCP16 was investigated in nude mice bearing 4T1 (mouse mammary tumor cell line) tumors (n = 4 mice) (1). Two animals were intravenously injected with Gd-DCCP16 control, and the other two animals were injected with Gd-DCCP16. Images were acquired at 9.4 T before, immediately after, and 24 h after injection. The relaxation rate (R_1_) was elevated in all tumors immediately after injection, but high R_1_ was observed only for Gd-DCCP16 at 24 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Tei L., Mazooz G., Shellef Y., Avni R., Vandoorne K., Barge A., Kalchenko V., Dewhirst M.W., Chaabane L., Miragoli L., Longo D., Neeman M., Aime S. (2010). Novel MRI and fluorescent probes responsive to the Factor XIII transglutaminase activity. Contrast Media Mol Imaging.
2 Bergamini C.M., Griffin M., Pansini F.S. (2005). Transglutaminase and vascular biology: physiopathologic implications and perspectives for therapeutic interventions. Curr Med Chem.
3 Park D., Choi S.S., Ha K.S. (2010). Transglutaminase 2: a multi-functional protein in multiple subcellular compartments. Amino Acids.
4 Aeschlimann D., Thomazy V. (2000). Protein crosslinking in assembly and remodelling of extracellular matrices: the role of transglutaminases. Connect Tissue Res.
5 McCarthy J.R., Patel P., Botnaru I., Haghayeghi P., Weissleder R., Jaffer F.A. (2009). Multimodal nanoagents for the detection of intravascular thrombi. Bioconjug Chem.
6 Jaffer F.A., Tung C.H., Wykrzykowska J.J., Ho N.H., Houng A.K., Reed G.L., Weissleder R. (2004). Molecular imaging of factor XIIIa activity in thrombosis using a novel, near-infrared fluorescent contrast agent that covalently links to thrombi. Circulation.
7 Mehta K., Kumar A., Kim H.I. (2010). Transglutaminase 2: a multi-tasking protein in the complex circuitry of inflammation and cancer. Biochem Pharmacol.
8 Wilhelmus M.M., van Dam A.M., Drukarch B. (2008). Tissue transglutaminase: a novel pharmacological target in preventing toxic protein aggregation in neurodegenerative diseases. Eur J Pharmacol.
9 Collighan R.J., Griffin M. (2009). Transglutaminase 2 cross-linking of matrix proteins: biological significance and medical applications. Amino Acids.
10 Miserus R.J., Herias M.V., Prinzen L., Lobbes M.B., Van Suylen R.J., Dirksen A., Hackeng T.M., Heemskerk J.W., van Engelshoven J.M., Daemen M.J., van Zandvoort M.A., Heeneman S., Kooi M.E. (2009). Molecular MRI of early thrombus formation using a bimodal alpha2-antiplasmin-based contrast agent. JACC Cardiovasc Imaging.
11 Mazooz G., Mehlman T., Lai T.S., Greenberg C.S., Dewhirst M.W., Neeman M. (2005). Development of magnetic resonance imaging contrast material for in vivo mapping of tissue transglutaminase activity. Cancer Res.
12 Caccamo D., Curro M., Ientile R. (2010). Potential of transglutaminase 2 as a therapeutic target. Expert Opin Ther Targets.